# ^99m^Tc-Labeled acetylated dendrimer poly(amido)-amine generation 5-PEGylated folic acid-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid conjugate

Chemical name: | ^99m^Tc-Labeled acetylated dendrimer poly(amido)-amine generation 5-PEGylated folic acid-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid conjugate
Abbreviated name: | ^99m^Tc-G5-Ac-pegFA-DTPA
Synonym:
Agent Category: | Compounds
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=folate+and+dendrimer+and+imaging)]

^99m^Tc-Labeled acetylated (Ac) dendrimer poly(amido)-amine (PAMAM) generation 5 (G5)-PEGylated folic acid (FA)-2-(p-isothiocyanatobenzyl)-6-methyl-diethylenetriamine pentaacetic acid (1B4M DTPA) conjugate, abbreviated as ^99m^Tc-G5-Ac-pegFA-DTPA, was synthesized by Zhang et al. for folate receptor (FR)-targeted imaging of FR-positive tumors (1, 2).

Folate is an essential vitamin for cell synthesis of nucleotide bases. Some unique features of the FR-folate system make it extremely valuable for developing FR-targeted imaging and therapeutic agents (3-5). First, FR has a high affinity for the exogenous folate conjugates (K_d_ = ~100 pM), but they are inaccessible for the conjugates in most normal tissues. Second, FR-α isoform is overexpressed on ~40% of human cancers, where it is completely accessible to folate conjugates. Third, folate conjugates are taken up by cancer cells via FR-mediated endocytosis, and FR recycles actively to the cell surface with a frequency of 5.7–20 h depending on cell types. Fourth, conjugation of imaging labels via the γ-carboxyl group of folate has no apparent effects on the ligand-binding affinity to FR. Furthermore, folate is a small molecule (MW = ~441) that exhibits rapid and complete penetration of solid tumors and rapid clearance from FR-negative tissues (t_1/2_, <10 min). One disadvantage of the FR-folate system is that FR expresses at a relatively low density on some tumor cell surface (1–3 million FR/cell), which means that the FR-folate binding can be saturated rapidly and the imaging contrast will be limited (3, 4, 6). Sensitive imaging techniques such as positron emission tomography and single-photon emission computed tomography (SPECT) are more desirable for FR-targeted imaging (3, 4, 7). To date, a large set of folate-based radiopharmaceutical agents have been synthesized for nuclear imaging (8). In general, a chelating agent is necessary to bridge the radiolabels and the folate molecule. The chelating agent is also critical for optimizing the molecular properties of conjugates (1, 2, 9).

Dendrimers represent a unique class of nanostructures that are synthesized from branched monomers in a step-wise manner. The molecular properties of dendrimers can be precisely controlled by choosing different branching monomers and surface functional groups (1, 2, 9). PAMAM is one of the most extensively studied dendrimers. Zhang et al. synthesized two folate-based compounds, ^99m^Tc-G5-Ac-pegFA-DTPA and ^99m^Tc-G5-Ac-FA-DTPA, and one control, ^99m^Tc-G5-Ac-DTPA, with PAMAM G5 dendrimer and folate (1, 2). To increase the solubility and decrease the nonspecific cellular uptake of the agents, the primary amines on the surface of PAMAM dendrimers were partially converted to acetamide moieties, which were used to link with the bifunctional chelating agent 1B4M DTPA. Folate was either PEGylated or left unPEGylated, and its c-carboxyl group was used to conjugate with the primary amine of PAMAM. The two folate-based conjugates exhibited excellent stability, rapid clearance from blood, and high accumulation in tumor xenografts (1, 2). This chapter describes the results obtained with ^99m^Tc-G5-Ac-pegFA-DTPA. Another chapter in MICAD describes the data obtained with ^99m^Tc-G5-Ac-FA-DTPA (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- FR-targeted chapters (http://www.ncbi.nlm.nih.gov/books/?term=folate%20receptor%20AND%20micad%5bbook%5d) on MICAD
- Protein (http://www.ncbi.nlm.nih.gov/protein/?term=Folate+Receptor) and nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Folate+Receptor) information of FR
- FR-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=Folate+Receptor) in Clinicaltrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

Zhang et al. described the synthesis of ^99m^Tc-G5-Ac-pegFA-DTPA, ^99m^Tc-G5-Ac-FA-DTPA, and ^99m^Tc-G5-Ac-DTPA (1, 2). The primary amines on the surface of G5 PAMAM dendrimers were first partially converted to acetamide moieties (G5-Ac, yield = 94.7%). PEGylated folate (NHS-PEG1540-FA) was synthesized through reactions of N-hydroxysuccinimide ester of FA with poly(ethylene glycol)bis amine (NH_2_-PEG1540-NH_2_). Conjugation of the folate or PEGylated folate to the dendrimers was achieved via condensation between the γ-carboxyl group of folate and the remaining primary amine of dendrimer (G5-Ac-FA or G5-Ac-pegFA, yield = 90.8%). The partially acetylated dendrimers were then linked with the chelating agent 1B4M DTPA to generate G5-Ac-FA-DTPA, G5-Ac-pegFA-DTPA, or G5-Ac-DTPA (yield = 98.2%). Each G5-Ac-DTPA contained 77 acetyl and 8 DTPA molecules. Each G5-Ac-FA-DTPA contained 77 acetyl, 4.8 folic acid molecules, and 7 DTPA molecules, and each G5-Ac-pegFA-DTPA contained 77 acetyl, 5.2 folic acid molecules, and 8 DTPA molecules. Therefore, the three compounds (G5-Ac-pegFA-DTPA, G5-Ac-FA-DTPA, and G5-Ac-DTPA) contained a similar number of DTPA molecules (i.e., 7 to 8 molecules). The two folate conjugates (G5-Ac-pegFA-DTPA and G5-Ac-FA-DTPA) contained a similar number of folic acid molecules (i.e., 4.8 to 5.2 molecules).

Radiolabeling was performed after reduction of ^99m^TcO4− to reduced ^99m^Tc using stannous chloride. The radiochemical yield and radioactivity of the three radiolabeled agents were >95% and 88.3 ± 1.0%, respectively. They were used for experiments without further purification. The partition ratios (log P) between n-octanol and water were −2.030, −2.061, and −2.167 for ^99m^Tc-G5-Ac-FA-DTPA, ^99m^Tc-G5-Ac-pegFA-DTPA, and ^99m^Tc-G5-Ac-DTPA, respectively, indicating that the agents had high water solubility. No specific activity was recorded.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

The in vitro stability was analyzed after incubation of the ^99m^Tc-G5-Ac-FA-DTPA, ^99m^Tc-G5-Ac-pegFA-DTPA, and ^99m^Tc-G5-Ac-DTPA with phosphate-buffered saline and new-born calf serum, respectively. After incubation for 6 h at 37ºC, at least 86% and 84% of the agents kept their original structure in phosphate-buffered saline and in new-born calf serum, respectively, indicating high stability.

Cell uptake of the three agents was quantitatively measured with FR-expressing KB cells (a human oral epidermoid carcinoma line) (1, 2). In vitro cell binding of the ^99m^Tc-G5-Ac-pegFA-DTPA was ~15% of total added radioactivity after incubation for 6 h at 37ºC, whereas ^99m^Tc-G5-Ac-FA-DTPA and the control ^99m^Tc-G5-Ac-DTPA exhibited lower binding ability (~11% and ~10%, respectively).

These results indicated that conjugation of FA directly to PAMAM dendrimers did not improve the cell uptake. In contrast, conjugation through a PEG spacer could improve the cellular internalization. Uptake of the three agents in the KB cells grown in FA-rich medium (to inhibit FR expression) was similar (<10%), suggesting no significant binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20350006)]

The in vivo studies on stability after injection into mice (n = 3/time point) showed that 80.78% of the ^99m^Tc-G5-Ac-pegFA-DTPA and 80.56% of the ^99m^Tc-G5-Ac-DTPA remained as the parent compound within 6 h in blood of normal mice (1, 2).

The pharmacokinetics of the agents was studied in normal mice (n = 5) (1, 2). A rapid decrease was observed at 30 min after injection, followed by a slow clearance. The plasma half-life was estimated to be 13.15 min for ^99m^Tc-G5-Ac-pegFA-DTPA and 12.73 min for the control ^99m^Tc-G5-Ac-DTPA. Less than 10% of the injected agents remained in circulation after 6 h (assuming that blood represents 5.5% of the total body mass).

Biodistribution was investigated with KB tumor–bearing nude mice (n = 3/time point). The mice were maintained on a folate-deficient diet for the duration of the experiment to minimize the circulating levels of FA. ^99m^Tc-G5-Ac-pegFA-DTPA was cleared rapidly from the blood, decreasing from 11.52% injected dose/gram (ID/g) at 2 h to 4.37% ID/g at 6 h. In the organs known not to express FR, the uptake of the conjugate remained at a low level. Both ^99m^Tc-G5-Ac-DTPA and ^99m^Tc-G5-Ac-FA-DTPA showed similar clearance from blood and uptake in the FR-negative organs. The concentrations of the three agents in the brain were low at all time points, suggesting that the dendrimer conjugates could not cross the blood–brain barrier.

The kidneys, which express FR, are the major clearance organs. The level of nontargeted ^99m^Tc-G5-Ac-DTPA decreased from 32.08% ID/g at 2 h to 26.06% ID/g at 6 h. In contrast, the level of ^99m^Tc-G5-Ac-pegFA-DTPA increased with time (18.21% ID/g at 2 h to 28.82% ID/g at 6 h). In the liver, the concentrations of nontargeted ^99m^Tc-G5-Ac-DTPA decreased with clearance from blood (41.07% ID/g at 2 h to 32.94% ID/g at 6 h), whereas the targeted ^99m^Tc-G5-Ac-pegFA-DTPA decreased more slowly (28.93% ID/g at 2 h to 22.23% ID/g at 6 h). In the tumors, the level of ^99m^Tc-G5-Ac-pegFA-DTPA increased from 3.82% ID/g at 2 h to 10.27% ID/g at 6 h. The nontargeted ^99m^Tc-G5-Ac-DTPA also increased slightly from 2.81% ID/g at 2 h to 4.38% ID/g at 6 h.

Micro-SPECT imaging confirmed the predominant uptake of ^99m^Tc-G5-Ac-pegFA-DTPA in the FR-positive tumors, liver, and kidneys in the KB tumor–bearing mice (n = 2/time point).

In conclusion, PEGylation of the PAMAM dendrimer-FA conjugate improves the tumor targeting and may be used as a targeted delivery system for imaging labels (1, 2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Zhang Y., Sun Y., Xu X., Zhu H., Huang L., Zhang X., Qi Y., Shen Y.M. (2010). Radiosynthesis and micro-SPECT imaging of 99mTc-dendrimer poly(amido)-amine folic acid conjugate. Bioorg Med Chem Lett.
2 Zhang Y., Sun Y., Xu X., Zhang X., Zhu H., Huang L., Qi Y., Shen Y.M. (2010). Synthesis, biodistribution, and microsingle photon emission computed tomography (SPECT) imaging study of technetium-99m labeled PEGylated dendrimer poly(amidoamine) (PAMAM)-folic acid conjugates. J Med Chem.
3 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
4 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
5 Zhao X., Li H., Lee R.J. (2008). Targeted drug delivery via folate receptors. Expert Opin Drug Deliv.
6 Miotti S., Bagnoli M., Ottone F., Tomassetti A., Colnaghi M.I., Canevari S. (1997). Simultaneous activity of two different mechanisms of folate transport in ovarian carcinoma cell lines. J Cell Biochem.
7 Altiparmak B., Lambrecht F.Y., Bayrak E., Durkan K. (2010). Design and synthesis of 99mTc-citro-folate for use as a tumor-targeted radiopharmaceutical. Int J Pharm.
8 Low P.S., Henne W.A., Doorneweerd D.D. (2008). Discovery and development of folic-acid-based receptor targeting for imaging and therapy of cancer and inflammatory diseases. Acc Chem Res.
9 Konda S.D., Aref M., Wang S., Brechbiel M., Wiener E.C. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. MAGMA.